# ^111^In-Labeled annexin A5-polyethylene glycol–coated core-cross-linked polymeric micelle-Cy7

Chemical name: | ^111^In-Labeled annexin A5-polyethylene glycol–coated core-cross-linked polymeric micelle-Cy7
Abbreviated name: | ^111^In-A5-CCPM
Synonym:
Agent category: | Protein
Target: | Phosphatidylserine, apoptosis
Target category: | Phospholipid
Method of detection: | Multimodality imaging: SPECT, planar gamma imaging; optical (near-infrared (NIR) fluorescence)
Source of signal\contrast: | ^111^In, Cy7
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=468888), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4809273) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=308) for more information about annexin V.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20A5%20and%20micelles)]

Apoptosis (programmed cell death) plays an important role in the pathophysiology of many diseases, such as cancers, neurodegenerative disorders, vascular disorders, atherosclerosis, and chronic hepatitis, as well as in the biology of normal cells like epithelial cells and immune cells (1). During apoptosis, there is rapid redistribution of phosphatidylserine (PS) from the inner membrane leaflet to the outer membrane leaflet, exposing the anionic head group of PS. PS is also accessible for annexin V (or annexin A5) binding in necrosis because of disruption of the plasma membrane. Annexin V, a 36-kDa protein, binds to PS with high affinity (K_d_ = 7 nM). Annexin V derivatives have been developed for imaging apoptosis as well as necrosis with different imaging modalities such as single-photon emission computed tomography (SPECT) (2-4), positron emission tomography (5), near-infrared (NIR) fluorescence (6), and magnetic resonance imaging (7).

Cy5.5-Annexin V has been evaluated as an optical probe in small animals. Annexin V-CLIO-Cy5.5 (AnxCLIO-Cy5.5 (http://www.ncbi.nlm.nih.gov/books/NBK23475/)) is a multimodal agent that consists of CLIO nanoparticles labeled with annexin V and Cy5.5 (6). van Tilborg et al. (7) incorporated annexin A5 into di-stearoyl-polyethylene glycol-phosphatidylethanolamine 2000 (DSPE-PEG2000) micelles labeled with gadolinium-labeled diethylenetriamine pentaacetic acid (Gd-DTPA) and Cy5.5 (annexin A5-Gd-micelles-Cy5.5) for multimodality imaging of atherosclerotic plaques. Zhang et al. (8) conjugated A5 to PEG-coated core-cross-linked polymeric micelles (CCPMs) labeled with Cy7 and ^111^In (^111^In-A5-CCPM) for multimodality detection of apoptosis in tumor-bearing mice.

### Related Resource Links:

- Chapters in MICAD (Annexin V (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Annexin%20V+AND+micad%5Bbook%5D))
- Gene information in NCBI (Annexin V (http://www.ncbi.nlm.nih.gov/gene/308))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Annexin V (http://www.ncbi.nlm.nih.gov/omim/131230))
- Clinical trials (Annexin V (http://www.clinicaltrials.gov/ct2/results?term=Annexin+V+))
- Drug information in FDA (Annexin V (http://google2.fda.gov/search?q=annexin+V&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=3&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20A5%20micelles%20and%20synthesis)]

CCPM nanoparticles were obtained from Carestream Health (Rochester, NY). There were ~21 Cy7 dye molecules, 180 amino groups, and 19 DTPA moieties per CCPM nanoparticle. Annexin A5 was conjugated to the maleimide-CCPM by sulfhydryl-maleimide bonding. A5-CCPMs were purified with column chromatography (8). The average hydrodynamic diameter of A5-CCPMs was determined to be ~25 nm. There were 40 annexin A5 molecules per nanoparticle. The maximum excitation and emission intensities were 755 nm and 781 nm, respectively. ^111^In-A5-CCPM was prepared by incubation of A5-CCPM with ^111^InCl_3_ in sodium acetate buffer (pH 5.2) for 30 min at room temperature with a labeling efficiency of >98%. The specific activity was 185 MBq/nmol (5 mCi/nmol). Control ^111^In-CCPMs without annexin A5 were prepared similarly with similar quality control metrics.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20A5%20micelles%20and%20in%20vitro)]

Zhang et al. (8) performed cell-binding assays with ^111^In-A5-CCPM and ^111^In-CCPM in apoptotic and normal viable human DLD-1 colon cancer cells with the use of fluorescence microscopy and radioactivity measurements at 2 h after incubation. The apoptotic cells (25% apoptotic) incubated with ^111^In-A5-CCPM (1.8 MBq/ml) showed clear cell-associated fluorescence and radioactivity signals, whereas negligible signals were obtained with control ^111^In-CCPM. Normal cells (3% apoptotic) showed little signal with ^111^In-A5-CCPM. Both signals in the apoptotic cells treated with ^111^In-A5-CCPM were blocked to background levels by 100-fold excess A5.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20A5%20micelles%20and%20rodentia)]

Zhang et al. (8) performed ex vivo biodistribution studies in mice bearing EL-4 lymphoma tumors with or without cyclophosphamide and etoposide treatment to induce apoptosis. ^111^In-A5-CCPM (1 x 10^14^ nanoparticles, 9.2 MBq/mouse), ^111^In-CCPM, or ^99m^Tc-HYNIC-A5 was injected intravenously in the mice at 24 h after drug treatment (n = 5-7/group). At 48 h after injection, ^111^In-A5-CCPM exhibited significantly higher accumulation in the tumors (8.0% injected dose/gram (ID/g)) and spleens (20% ID/g) of the treated mice than in the tumors (3.2% ID/g) and spleens (13% ID/g) of untreated mice (P < 0.001). The tumor/muscle ratios were 14.8 and 38.8 for the untreated mice and treated mice, respectively. The livers of both groups accumulated ~9% ID/g. The accumulation levels in other normal tissues (<2% ID/g) were similar in both treated and untreated mice. ^111^In-A5-CCPM showed significantly (P < 0.001) higher tumor accumulation in the tumors of the treated mice than ^111^In-CCPM (2.8% ID/g, 48 h after injection) and ^99m^Tc-HYNIC-A5 (4.1% ID/g, 6 h after injection). Autoradiography and immunohistochemistry showed that the fluorescence and nuclear signals of ^111^In-A5-CCPM co-localized with caspase-3 in the tumor sections from mice treated with cyclophosphamide and etoposide. No blocking studies were performed.

SPECT and optical imaging scans were performed in mice (n = 2-4/group) bearing EL-4 lymphoma tumors with or without cyclophosphamide and etoposide treatment at 48 h after injection of 9.2 MBq (0.25 mCi) ^111^In-A5-CCPM. The apoptotic tumors were clearly visualized in the treated mice with SPECT and NIR fluorescence imaging, but little signal was detected in the tumors of untreated mice with these imaging modalities. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20A5%20micelles%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20A5%20micelles%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20A5%20micelles%20and%20human)]

No publication is currently available.

## NIH Support

R01 CA119387, RC2 GM092599, CA016672

## References

1 Thompson C.B. (1995). Apoptosis in the pathogenesis and treatment of disease. Science.
2 Blankenberg F.G. (2004). Recent advances in the imaging of programmed cell death. Curr Pharm Des.
3 Keen H.G., Dekker B.A., Disley L., Hastings D., Lyons S., Reader A.J., Ottewell P., Watson A., Zweit J. (2005). Imaging apoptosis in vivo using 124I-annexin V and PET. Nucl Med Biol.
4 Lahorte C., Slegers G., Philippe J., Van de Wiele C., Dierckx R.A. (2001). Synthesis and in vitro evaluation of 123I-labelled human recombinant annexin V. Biomol Eng.
5 Murakami Y., Takamatsu H., Taki J., Tatsumi M., Noda A., Ichise R., Tait J.F., Nishimura S. (2004). 18F-labelled annexin V: a PET tracer for apoptosis imaging. Eur J Nucl Med Mol Imaging.
6 Schellenberger E.A., Sosnovik D., Weissleder R., Josephson L. (2004). Magneto/optical annexin V, a multimodal protein. Bioconjug Chem.
7 van Tilborg G.A., Mulder W.J., Deckers N., Storm G., Reutelingsperger C.P., Strijkers G.J., Nicolay K. (2006). Annexin A5-functionalized bimodal lipid-based contrast agents for the detection of apoptosis. Bioconjug Chem.
8 Zhang R., Lu W., Wen X., Huang M., Zhou M., Liang D., Li C. (2011). Annexin A5-conjugated polymeric micelles for dual SPECT and optical detection of apoptosis. J Nucl Med.